# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidethylacetamide-Ac-Cys-Z_EGFR:1907_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidethylacetamide-Ac-Cys-Z_EGFR:1907_
Abbreviated name: | ^64^Cu-DOTA-Z_EGFR:1907_
Synonym: | ^64^Cu-DO3A-Z_EGFR:1907_
Agent category: | Antibody, Affibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells, such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use in anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2, based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A, was constructed (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. The EGFR-specific Affibody Z_EGFR:1907_ (6.7 kDa) was identified to have good affinity (K_d_ = 5.4 nM) for EGFR (HER1) and was labeled with ^111^In via isothiocyanate-benzoyl-diethylenetriamine pentaacetic acid (DTPA) to form ^111^In-Bz-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/) for single-photon emission computed tomography (18) imaging in nude mice bearing human tumors (19). To facilitate site-specific conjugation, Ac-Cys-Z_EGFR:1907_ (Cys at the N terminal) was synthesized and conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidethylacetamide (maleimido-mono-amide-DOTA) to form Ac-Cys(DOTA)-Z_EGFR:1907_ (DOTA-Z_EGFR:1907_), and the product was labeled with ^64^Cu (t_1/2_, 12.7 h) to form ^64^Cu-DOTA-Z_EGFR:1907_ for positron emission tomography (PET) imaging studies in tumor-bearing mice (20).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR+1907+synthesis)]

Ac-Cys-Z_EGFR:1907_ was prepared with an automated solid-phase peptide synthesizer (20). Maleimido-mono-amide-DOTA and Ac-Cys-Z_EGFR:1907_ (20:1 molar ratio) were incubated in phosphate buffer (pH 7.4) for 2 h at 25°C. DOTA-Z_EGFR:1907_ was isolated with high-performance liquid chromatography (HPLC), with 47% recovery yield and >95% purity. Chemical and mass spectroscopy analysis confirmed 1:1 DOTA conjugation. DOTA-Z_EGFR:1907_ in 0.1 N sodium acetate buffer (pH 6.3) was mixed with a predetermined amount of ^64^CuCl_2_. The mixture was incubated for 1 h at 45°C, with a labeling efficiency of >50%. ^64^Cu-DOTA-Z_EGFR:1907_ was purified with PD-10 column chromatography, with a radiochemical purity of >95% as measured with HPLC. The specific activity of ^64^Cu-DOTA-Z_EGFR:1907_ was 5–8 MBq/nmol (0.14–0.22 mCi/nmol) at the end of synthesis. ^64^Cu-DOTA-Z_EGFR:1907_ exhibited a moderate hydrophilicity, with a log P value of −1.01 ± 0.09. ^64^Cu-DOTA-Z_EGFR:1907_ was >95% intact after incubation in mouse serum for 4 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20in%20vitro)]

In vitro binding specificity tests showed that binding of ^64^Cu-DOTA-Z_EGFR:1907_ to A431 human epidermoid carcinoma cells expressing EGFR was mediated by the receptors because saturation of receptors by incubation with non-labeled Ac-Cys-Z_EGFR:1907_ significantly decreased binding of ^64^Cu-DOTA-Z_EGFR:1907_ (20). The cell-bound radioactivity remained >20% of the initially bound activity for up to 2 h at 37°C. ^64^Cu-DOTA-Z_EGFR:1907_ exhibited a K_d_ value of 20 nM for the EGFR of A431 cells as measured with saturation assay at 4°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20rodentia)]

Miao et al. (20) performed ex vivo biodistribution studies of 1.11–1.85 MBq (0.03–0.05 mCi, 0.14–0.28 nmol) ^64^Cu-DOTA-Z_EGFR:1907_ in nude mice (n = 3/group) bearing A431 xenografts at 4 h after injection. Co-injection of 0, 0.69, 6.9, and 69 nmol unlabeled Ac-Cys-Z_EGFR:1907_ produced tumor accumulation of 11.71% injected dose per gram (ID/g), 11.02% ID/g, 17.35% ID/g, and 6.15% ID/g, respectively. The highest spiking dose blocked tumor accumulation by ~50%.The organ with the highest radioactivity was the kidney (88.40% ID/g), followed by the liver (18.99% ID/g) and blood (11.68% ID/g), as observed with no spiking cold dose of Ac-Cys-Z_EGFR:1907_. The radioactivity levels in the other tissues were lower than that of the tumor. In general, the highest spiking dose decreased the accumulation levels in most normal tissues except the kidney. Blood levels were 11.69% ID/g, 4.84% ID/g, 1.81% ID/g, and 1.15% ID/g for 0, 0.69, 6.9, and 69 nmol Ac-Cys-Z_EGFR:1907_, respectively.

PET imaging analysis was performed in nude mice bearing A431 tumors at 1, 2, 4, and 24 h after intravenous injection of 1.11–1.85 MBq (0.03–0.05 mCi, 0.14–0.28 nmol) ^64^Cu-DOTA-Z_EGFR:1907_ with or without co-injection of 0.69, 6.9, and 69 nmol unlabeled Ac-Cys-Z_EGFR:1907_ (20). At a spiking dose of 0 nmol, the tumor was only clearly visualized at 2 h after injection. At a spiking dose of 0.69 nmol, the tumor was clearly visualized at 2–24 h. At a spiking dose of 6.9 nmol, the tumor was clearly visualized at 1–4 h. At a spiking dose of 69 nmol, the tumor was not visualized at 1–4 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Goldman E.R., O'Shaughnessy T.J., Soto C.M., Patterson C.H., Taitt C.R., Spector M.S., Charles P.T. (2004). Detection of proteins cross-linked within galactoside polyacrylate-based hydrogels by means of a quantum dot fluororeagent. Anal Bioanal Chem.
19 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
20 Miao Z., Ren G., Liu H., Jiang L., Cheng Z. (2010). Small-animal PET imaging of human epidermal growth factor receptor positive tumor with a 64Cu labeled affibody protein. Bioconjug Chem.